# ^111^In-Labeled chimeric monoclonal antibody, ch806, targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)

Chemical name: | ^111^In-Labeled chimeric monoclonal antibody, ch806, targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Abbreviated name: | [^111^In]-ch806
Synonym: | [^111^In]-CHX-A”-DTPA-ch806
Agent Category: | Antibody
Target: | Epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Human Studies | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, and functioning of the different members of the transmembrane epidermal growth factor receptor (EGFR) family are described elsewhere (1-3). The EGFR receptors are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signal transduction pathway, and they are overexpressed in many malignant epithelial tumors (1, 2). Overexpression of the EGFR in tumors has been attributed to gene amplification, and this phenomenon is believed to introduce mutations in the receptor (2, 4). Also, overexpression of the EGFR usually indicates a poor clinical prognosis for the patient (4). The most common mutation observed in the EGFR receptor is the deletion of a segment of the extracellular domain, including the ligand-binding region, which results in the generation of a variant known as the de2-7 EGFR or EGFRvIII (2, 4). The generation, structure, functions, and role of the EGFRvIII in tumor malignancy have been reviewed by Gan et al. (5). Although the EGFRvIII is nonresponsive to the ligand, it is constitutively active with a constantly operating downstream TK signaling pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastomas and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain the cancerous state of cells, several antibodies that inhibit the receptor activity and small molecules that block the downstream TK signaling pathway have been developed and have been approved by the United States Food and Drug Administration (FDA) for the treatment of certain cancers (2). The antibodies are directed toward the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which ultimately results in downregulation of the EGFR on the cell surface. However, because the EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). As a consequence, the monoclonal antibody (mAb) 806, which specifically targets the EGFRvIII, was generated and characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated as ch806, was developed (9) and evaluated in a phase I clinical trial with patients having cancerous tumors overexpressing the EGFRvIII (4). Results obtained from this trial indicated that ch806 could be a good biotherapeutic agent for the treatment of cancers expressing the ch806 antigen (4). In addition, several other clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) approved by the FDA are in progress to evaluate the targeting of EGFRvIII as a treatment against various cancers.

The internalization, intracellular trafficking, and biodistribution (in nude mice bearing xenograft human epidermoid carcinoma cell tumors) of mAb806 labeled with ^125^I and ^111^In, respectively, have been investigated by Perera et al. (8) and are described separately in MICAD (www.micad.nih.gov) (10, 11). The characterization and biodistribution (in nude mice bearing xenograft human glioblastoma cell tumors) of ch806 labeled with ^125^I ([^125^I]-ch806) or ^111^In ([^111^In]-ch806) have been investigated by Panousis et al. (9). The use of ^124^I-labeled ch806 for the detection of EGFRvIII-expressing xenograft human glioblastoma tumors in nude mice with an immuno–positron emission tomography (PET) technique was investigated by Lee et al. (6) and has been described in another chapter in MICAD (12). This chapter describes the studies performed with [^111^In]-ch806. Studies performed with [^125^I]-ch806 are described in a separate chapter in MICAD (13).

### Other sources of information

Human EGFR Gene (http://www.ncbi.nlm.nih.gov/gene/1956) (Gene ID: 1956)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200131&source=NATURE&output-format=graphic&ppage=1&genes_a=1956) (NCI-Nature Pathways Interactive Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-CHX-A%u201D-DTPA-ch806%20synthesis&cmd=DetailsSearch)]

The production and labeling of ch806 to obtain [^111^In]-ch806 (as a ^111^In-labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans(S,S)-cyclohexane-1,2-diethylenetriamine pentaacetic acid (CHX-A''-DTPA) conjugate of ch806; [^111^In]-CHX-A”-DTPA-ch806 or [^111^In]-ch806) is described elsewhere (9). The radiochemical purity of [^111^In]-chAb was reported to be 98.6% as determined with instant thin-layer chromatography. The specific activity of [^111^In]-ch806 was reported to be 0.0840–0.1221 MBq/6.6 pmol (~422 Ci/mmol). The final formulation, the number of CHX-A”-DTPA per ch806 and storage conditions of the radiolabeled chAb were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-CHX-A-DTPA-ch806%20in%20vitro&cmd=DetailsSearch)]

The stability of [^111^In]-ch806 was determined in healthy human donor serum at 37°C and was reported to maintain a radiochemical purity of >95% for up to 7 days (9). Under the same storage conditions and duration, immunoreactivity of the labeled chAb with U87MG.de2-7 cells (a human glioma cell line generated to overexpress the EGFRvIII) was determined to be >65%. Using various cell lines expressing or overexpressing the EGFRvIII or the wild-type EGFR, respectively, it was shown that ch806 and the parental mAb806 had a similar receptor-binding profile.

The receptor association constant for [^111^In]-ch806 was determined to be 1.36 × 10^9^ M^-1^ compared with 1.1 × 10^9^ M^-1^ for the parental mAb806 with the Lindmo assay using U87MG.de2-7 cells (9). The number of [^111^In]-ch806 molecules bound per cell was reported to be 6.0 × 10^5^ compared with 4.7 × 10^5^ for the [^125^I]-labeled ch806 (9).

In a clinical study using immunohistochemical techniques, 50% to 75% of cells in tumor samples from six of eight cancer patients were shown to bind ch806 (4). Cells of tumor samples obtained from the remaining two patients showed <10% binding of the chAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^111^In]-ch806 and [^125^I]-ch806 were studied in BALB/c nude mice respectively bearing xenograft U87MB.de2-7 and A431 cell tumors (of human epidermoid carcinoma origin; overexpress the EGFR and do not express the EGFR, respectively) (9). Nude mice bearing FaDu xenograft tumors (of human squamous cell carcinoma origin) were used as controls for this study. The animals (n = 3–5 animals/time point) were injected with the respectively labeled chAb through the tail vein and euthanized at predetermined time points ranging from 4 h to 312 h post-injection (p.i.) for the collection of tumors and all major organs (9). All data of radioactivity accumulated in the various organs were presented as percent of injected dose per gram tissue (% ID/g). In general, the uptake and retention of label by the tumors was significantly (P < 0.001) higher at all time points with [^111^In]-chAb806 (peaking at ~31.0% ID/g at 48 h) than with [^125^I]-ch806 (peaking at ~7.0% ID/g at 24 h). With [^111^In]-ch806, the accumulated radioactivity in the xenografts from 72 h to 168 h p.i. was observed to be more than six times higher than that with [^125^I]-ch806 in the same period (9). During the entire study period, the accumulation of radioactivity from [^111^In]-ch806 and [^125^I]-ch806 in all major organs was ~10.0% ID/g except for the kidneys and blood. The accumulation of radioactivity in these organs correlated to the level of tracer present in the blood pool of the animals. Lower uptake of the label and similar tracer biodistribution patterns were observed in all of the tissues from animals bearing the A431 or the FaDu xenograft tumors. No blocking studies using unlabeled ch806, mAb806, or another suitable anti-EGFR mAb were reported.

From serum samples obtained from the tracer-injected animals, the half-life times of [^111^In]-chAb806 and [^125^I]-ch806 were determined to be 3.42 ± 0.92 h and 2.85 ± 0.24 h, respectively (9). The total serum clearance for [^111^In]-chAb806 was reported to be 0.045 ± 0.005 ml/h; total serum clearance for [^125^I]-ch806 was 0.063 ± 0.0003 ml/h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-CHX-A-DTPA-ch806%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-CHX-A-DTPA-ch806%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Human%20Studies&cmd=DetailsSearch)]

Scott et al. investigated the tumor targeting, biodistribution, and pharmacokinetic properties of [111In]-chAb806 in an open-label, dose-escalating phase I study with eight patients having different cancerous lesions of the lungs (five patients), brain (one patient), lymph nodes (one patient), and supraglottis (one patient) (4). The objectives and patient inclusion or exclusion criteria for the study are described elsewhere (4). Each individual enrolled in the clinical trial received one of the four dose levels (5, 10, 20, or 40 mg/m2) of the unlabeled chAb.

To study the tumor uptake and biodistribution of the labeled chAb, whole-body gamma imaging was performed on the patients on different days, starting at day 0 for up to day 7, after an intravenous infusion of [111In]-chAb806. Blood clearance of the radioactivity from the patients was gradual at all dose levels, and the biological half-life of the labeled chAb was determined to be 948.6 ± 378.6 h. The tracer was observed to be cleared through the reticuloendothelial system during the 1-week period after the infusion. The accumulation of radioactivity in the targeted lesions, including in the brain, was apparent in all patients at the different dose levels of unlabeled ch806 (4).

For details of results obtained from the pharmacokinetic and dosimetry studies of [111In]-ch806, see Scott et al. (4). Briefly, the pharmacokinetic and dosimetry studies showed that no particular normal tissues could be saturated by ch806 and that there was no dose-dependent clearance of the labeled chAb from the organs or body of the patients. At the end of the 30-day study period, an assessment of the clinical response of patients at all dose levels of unlabeled ch806 indicated that five patients had stable disease and three patients had progressive disease. One patient at the 40 mg/m2-dose level showed some shrinkage of the lesion but was confirmed to have progressive disease by the RECIST criteria (response evaluation criteria in solid tumors) (14) at the end of the study.

From this study, the investigators concluded that ch806 had a very high selectivity to target the EGFR in tumors. Further evaluation of this chAb to treat cancers is ongoing (4).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
2 Pines G., Kostler W.J., Yarden Y. Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Hasselbalch, B., U. Lassen, H.S. Poulsen, and M.T. Stockhausen, Cetuximab Insufficiently Inhibits Glioma Cell Growth Due to Persistent EGFR Downstream Signaling. Cancer Invest.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Panousis C., Rayzman V.M., Johns T.G., Renner C., Liu Z., Cartwright G., Lee F.T., Wang D., Gan H., Cao D., Kypridis A., Smyth F.E., Brechbiel M.W., Burgess A.W., Old L.J., Scott A.M. (2005). Engineering and characterisation of chimeric monoclonal antibody 806 (ch806) for targeted immunotherapy of tumours expressing de2-7 EGFR or amplified EGFR. Br J Cancer.
10 Chopra, A., [125I]-Labeled monoclonal antibody 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated monoclonal antibody 806 (mAb 806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., [124I]-Labeled residulizing ligand IMP-R4 conjugated chimeric monoclonal antibody ch806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [125I]-Labeled chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
14 Eisenhauer E.A., Therasse P., Bogaerts J., Schwartz L.H., Sargent D., Ford R., Dancey J., Arbuck S., Gwyther S., Mooney M., Rubinstein L., Shankar L., Dodd L., Kaplan R., Lacombe D., Verweij J. (2009). New response evaluation criteria in solid tumours: revised RECIST guideline (version 1.1). Eur J Cancer.